# [^11^C]-[N-Methyl]3-[(3-fluorophenyl)sulfonyl]-8-(4-methyl-1-piperazinyl)quinoline

Chemical name: | [^11^C]-[N-Methyl]3-[(3-fluorophenyl)sulfonyl]-8-(4-methyl-1-piperazinyl)quinoline
Abbreviated name: | [^11^C]-GSK215083
Synonym:
Agent Category: | Compound
Target: | 5-HT_6_ receptor (5-HT_6_R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on above structure for information on [^11^C]-GSK215083 in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=5-ht6%20receptor&cmd=DetailsSearch)]

Serotonin (5-hydroxytryptamine; 5-HT), a derivative of the tryptophan amino acid, is a low molecular weight neurotransmitter that plays an important role in the functioning of different physiological, cognitive, and emotional processes. Impairment of the serotonergic system is associated with psychiatric disorders, such as anxiety and depression, and neurological afflictions, such as Parkinson’s disease, Alzheimer’s disease, and epilepsy (1). The 5-HT mediates its biological activity through a group of seven receptors (5-HT_1-7_R) that are further classified into 14 distinct subtypes on the basis of their structure and pharmacological activity. Except for the 5-HT_3_R, which is a ligand-gated ion channel, all other 5-HTRs belong to the family of G-protein–coupled seven-transmembrane receptors (2). Radiolabeled tracers have been developed for use with positron emission tomography (PET) to study the different 5-HTR subtypes, and much information is available regarding only the 5-HT_1A_R, 5-HT_1B_R, 5-HT_2A_R, and 5-HT_4_R subtypes (3). Compared to the discovery of the other 5-HTR subtypes, the identification of 5-HT_6_R is fairly recent, and this receptor is located mostly in the limbic and cortical regions of the mammalian central nervous system (4). Although the exact mechanism of action of the 5-HT_6_R is not clear, there are indications that antagonists of this receptor reverse amnesia and improve cognitive and memory functions in individuals suffering from schizophrenia, Parkinson's disease, or Alzheimer’s disease (5). Therefore, it was imperative to develop a ligand that could be used to study the biological characteristics of this receptor.

Radioiodinated SB-258585 ([^125^I]-SB258585), a selective antagonist of the 5-HT_6_R, has been shown to have a high affinity for this receptor in membranes derived from rat or pig striatum and human caudate putamen (6). Autoradiography of rat brain sections exposed to [^125^I]-SB258585 revealed that the 5-HT_6_R was located primarily in the striatum, followed by the cerebral cortex; accumulation was lowest in the cerebellum of these animals. From this observation, the investigators concluded that the receptor was probably involved in cognition, memory, and locomotor control functions in the animals (7). In another study, [N-methyl]3-[(3-fluorophenyl)sulfonyl]-8-(4-methyl-1-piperazinyl)quinoline (GSK215083) was reported to have a 5-fold and >55-fold higher subnanomolar concentration affinity for the 5-HT_6_R compared to the concentrations required for the 5-HT_2A_R and the other 5-HTRs, respectively (3). In addition, the lipophilicity of GSK215083 was determined to be suitable for crossing the blood–brain barrier and penetration into the brain. On the basis of these observations, [^11^C]-GSK215083 was evaluated in vivo as a 5-HT_6_R ligand in pigs, non-human primates, and humans (3).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=5-HT+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Serotonin+receptors) on serotonin receptors

Protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_000871.1) sequences of human 5-HT_6_R

5-HT_6_R in Online Mendelian Inheritance in Man Database (OMIM) (http://omim.org/entry/601109)

Gene information (http://www.ncbi.nlm.nih.gov/gene/3362) for 5-HT_6_R; Gene ID: 3362

Drugs related (http://www.genome.jp/dbget-bin/get_linkdb?-t+drug+hsa:3350) to 5-HTR (from Kyoto Encyclopedia of Genes and Genomics)

Human serotonergic synapse pathway (http://www.genome.jp/kegg-bin/show_pathway?hsa04726) (from Kyoto Encyclopedia of Genes and Genomics)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK215083%20synthesis&cmd=DetailsSearch)]

The synthesis of GSK215083 has been described in a United States patent filed by Ahmed et al. (8). The ^11^C labeling of the compound has been described by Parker et al. (3). The total time to prepare the tracer was reported to be 40 min from the end of bombardment. The radiochemical yield of the labeling reaction was 35 ± 5%, and the labeled product had a radiochemical purity of >99%. At the end of synthesis, the specific activity of the labeled compound was 414 ± 143 BGq/μmol (11.178 ± 3.86 Ci/μmol) for the preparation used in pigs and non-human primates and 47.4 ± 20.3 GBq/μmol (1.27 ± 0.55 Ci/μmol) for the preparation used in humans.

The synthesis or source of [^3^H]-GSK215083 used in a rat dosimetry study was not reported (3). The radiochemical purity of the ^3^H-labeled compound was 99.4%, with a specific activity of 3.07 TBq/mmol (82.9 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK215083%20in%20vitro&cmd=DetailsSearch)]

From in vitro studies performed with HeLa cells that stably expressed a recombinant human 5-HT_6_R, it was determined that GSK215083 had a dissociation constant (K_i_) of 0.16 nM for this receptor and that its K_i_ for the 5-HT_2A_R was 0.79 nM (~5-fold higher than that for 5-HT_6_R) (3). For the other 5-HTRs, the K_i_ of GSK215083 was between 9.1 nM (for 5-HT_2B_R) and >10,000 nM (for 5-HT_7_R). From this study, the investigators concluded that GSK215083 could be a suitable ligand for characterization of the 5-HT_6_R.

The lipophilicity (distribution coefficient, log D) of GSK215083 was determined to be 2.25 ± 0.11, which is considered ideal to allow penetration of the compound into the brain and to study the distribution and characteristics of the 5-HT_6_R in this organ (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK215083%20rodentia&cmd=DetailsSearch)]

The dosimetry of [^3^H]-GKS215083 was studied in rats to determine the expected radiation dose to administer to human subjects (3). The animals (the number of animals used in this study was not reported) were given a single bolus of the labeled compound (the route of administration not mentioned), and the rodents were euthanized between 5 min and 120 min postinjection (p.i.) to assess the biodistribution of the tracer in the various tissues. On the basis of the data obtained from this study (data not presented in the publication), it was estimated that a dose of up to 370 MBq [^11^C]-GSK215083 (mass dose of <10 μg (0.025 μmol)) can be administered to human subjects. This amount of [^11^C]-GSK215083 would produce a committed effective dose exposure of 8.22 × 10−^3^ mSv/MBq in humans (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK215083%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

The in vivo uptake of [^11^C]-GSK215083 in the brains of two pigs was investigated with PET imaging (3). A baseline PET scan of the animals (under anesthesia) was obtained after an intravenous injection of the high specific activity tracer. Three other sequential scans were performed on the same animals during the day. For these scans, the pigs were injected with escalating doses of non-radioactive GSK215083 (0.005, 0.05, and 0.5 mg/kg body weight) 5 min before the probe was administered to the animals. From the PET images it was evident that maximum uptake of radioactivity was in the striatum region (caudate and putamen areas) of the brain, followed by moderate accumulation in the cortical region, and the lowest amount of tracer was detected in the cerebellum. The uptake of [^11^C]-GSK215083 in various regions of the brain peaked between 10 min (striatum region) and 20 min p.i. (cortex and cerebellum). There was a slow washout of radioactivity from the striatum, whereas the loss of label from the cortex and the cerebellum was comparatively faster. Blood samples taken from the animals showed that [^11^C]-GSK215083 was metabolized rapidly in the arterial plasma, and at 35 min p.i. the intact compound comprised only 50% of the total radioactivity as determined with radiographic high-performance liquid chromatography. When the animals were given increasing doses of unlabeled GSK215083 followed by an injection of [^11^C]-GSK215083, a dose-dependent decrease in specific binding of the radiolabeled compound was observed in the striatum and the cortex regions, whereas the cerebellum showed a relatively small decrease in accumulation of the probe.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK215083%20Non-Human%20Primates&cmd=DetailsSearch)]

The uptake of [^11^C]-GSK215083 in the brain of non-human primates (Papio anubis) was investigated as described by Parker et al. (3). A baseline scan from the animals (n = 6 animals; under anesthesia) was acquired after an intravenous injection of the high specific activity tracer. For a second scan later in the day, the animals were first administered unlabeled GSK215083 (0.0002–0.5 mg/kg body weight), and 30 min later the monkeys were injected with the radiolabeled probe. PET images obtained from the scans showed that the uptake of [^11^C]-GSK215083 in different regions of the brain of these animals peaked between 15 min and 20 min p.i. (accumulation of radioactivity in striatum > cortex > cerebellum). The striatal regions of the monkey brain had the slowest washout of the tracer as observed in the pig study described above.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK215083%20Human%20Studies&cmd=DetailsSearch)]

The in vivo biodistribution of [^11^C]-GSK215083 in the brain of healthy human volunteers (n = 4 subjects) was also investigated (3). A baseline PET scan was obtained from each individual after an intravenous bolus injection of the tracer (352 ± 12 MBq (9.5 ± 0.32 mCi)). Peak levels of the radiolabeled compound were observed in the brain of the individuals between 10 min and 20 min p.i. (accumulation of label in striatum > cortex > cerebellum), and the striatal regions showed the slowest washout of the tracer. These observations were similar to those obtained from the pig and monkey studies.

From these studies, it was concluded that [^11^C]-GSK215083 can be a useful radioligand to investigate 5-HT_6_R (3). However, the investigators cautioned that because GSK215083 also has a high affinity for 5-HR2_AR_ (the affinity for 5-HT_2A_R is ~5-fold lower than that for 5-HR_6_R), data obtained with this tracer will have to be examined carefully for correct interpretation of the results.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Paterson, L.M., B.R. Kornum, D.J. Nutt, V.W. Pike, and G.M. Knudsen, 5-HT radioligands for human brain imaging with PET and SPECT. Med Res Rev, 2011
2 Hutcheson J.D., Setola V., Roth B.L., Merryman W.D. (2011). Serotonin receptors and heart valve disease--it was meant 2B. Pharmacol Ther.
3 Parker C.A., Gunn R.N., Rabiner E.A., Slifstein M., Comley R., Salinas C., Johnson C.N., Jakobsen S., Houle S., Laruelle M., Cunningham V.J., Martarello L. (2012). Radiosynthesis and Characterization of 11C-GSK215083 as a PET Radioligand for the 5-HT6 Receptor. J Nucl Med.
4 Tassone A., Madeo G., Sciamanna G., Pisani A., Bonsi P. (2010). Electrophysiology of 5-HT6 receptors. Int Rev Neurobiol.
5 Meneses A., Perez-Garcia G., Ponce-Lopez T., Castillo C. (2011). 5-HT6 receptor memory and amnesia: behavioral pharmacology--learning and memory processes. Int Rev Neurobiol.
6 Hirst W.D., Minton J.A., Bromidge S.M., Moss S.F., Latter A.J., Riley G., Routledge C., Middlemiss D.N., Price G.W. (2000). Characterization of [(125)I]-SB-258585 binding to human recombinant and native 5-HT(6) receptors in rat, pig and human brain tissue. Br J Pharmacol.
7 Roberts J.C., Reavill C., East S.Z., Harrison P.J., Patel S., Routledge C., Leslie R.A. (2002). The distribution of 5-HT(6) receptors in rat brain: an autoradiographic binding study using the radiolabelled 5-HT(6) receptor antagonist [(125)I]SB-258585. Brain Res.
8 Ahmed, M., C.N. Johnson, M.C. Jones, G.J. MacDonald, S.F. Moss, M. Thompson, C.E. Wade, and D. WittyQuinoline derivatives and their use as 5-HT6 ligands. Patent Number 7,977,337 United States Patent and Trademark Office, 2011, Glaox Group Limited USA.